# ^111^In-(Diethylenetriamine pentaacetic acid)_n_-trastuzumab-(IRDye 800CW)_m_

Chemical name: | ^111^In-(Diethylenetriamine pentaacetic acid)_n_-trastuzumab-(IRDye 800CW)_m_
Abbreviated name: | ^111^In-(DTPA)_n_-trastuzumab-(IRDye 800CW)_m_
Synonym:
Agent Category: | Antibody
Target: | Epidermal growth factor receptor 2 (EGFR2/neu)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT) or gamma planar imaging; near infrared fluorescence imaging
Source of signal / contrast: | ^111^In and IRDye 800CW
Activation: | No
Studies: | - In vitro; - Rodents | No structure available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+trastuzumab+IRDye800)]

The human epidermal growth factor receptor 2 (HER2), also known as neu, ErbB-2, or cluster of differentiation 340 (CD340), has a crucial role in the normal development, proliferation, survival, and apoptosis of the cell (1). HER2 is a tyrosine kinase (TK)-dependent receptor and regulates its own expression through the TK signaling pathway. An amplified expression of HER2 has been reported in 20–25% of breast cancer primary tumors and indicates a poor prognosis for the patient (2). Because of its role in the progression of cancer, HER2 or its associated TK are targeted either with antibodies or with small-molecule drugs (or a combination of the two) for the treatment of this ailment (3, 4). One of these antibodies, trastuzumab, which is a humanized monoclonal antibody (MAb) that targets the extracellular domain of the HER2, is approved (http://www.fda.gov/cder/foi/label/2008/103792s5175lbl.pdf) by the United States Food and Drug Administration for the treatment of breast cancer and is being evaluated in clinical trials (http://clinicaltrials.gov/ct2/results?term=Herceptin) for the treatment of several cancer types. Trastuzumab has also been conjugated with different radionuclides or fluorescent compounds and has been used under preclinical conditions for the diagnosis of breast cancer with different imaging techniques (5-7). In addition, this MAb has also been conjugated to gold nanoparticles (8), quantum dots (9), iron oxide (10), and nanocrystals (11) for the detection of cancer.

The use of MAbs for imaging after conjugation to either radionuclides or fluorescent dyes has its limitations. Radionuclide gamma ray emissions can penetrate tissue thereby permitting external detection, but have a physical half-life, and, therefore non-invasive imaging must be performed within a certain time period before the signal becomes difficult to detect or is limiting (12). Though fluorescent compounds do not have half-lives, deep tissue targets in humans may not be visible because of adsorption, but, compared with radionuclides, fluorescent compounds yield higher signal/noise ratios ex vivo that can assist in visualizing cancerous tissue during surgical resection (12). On the basis of these observations, Sampath et al. developed a dual-labeled trastuzumab-based imaging agent for the detection of HER2 expression in breast cancer tissue (12). The investigators synthesized radioactive indium (^111^In) and IRDye dual-labeled trastuzumab (^111^In-diethylenetriamine pentaacetic acid [DTPA])_n_-trastuzumab-(IRDye 800CW)_m_ or ^111^In-trastuzumab-IRDye 800CW) and used it for in vivo scintigraphic and fluorescent imaging of HER2-positive tumors in athymic nude mice bearing xenograft tumors.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+trastuzumab+IRDye800+synthesis)]

Sampath et al. described the synthesis of ^111^In-trastuzumab-IRDye 800CW (12). Trastuzumab and IRDye 800CW were obtained from commercial sources. The MAb was conjugated with DTPA as described by Tang et al. (13). The yield of this reaction was typically 98%. As determined with mass spectroscopy, 10 molecules (n) of DTPA were reported to be conjugated to each molecule of trastuzumab to yield (DTPA)_n_-trastuzumab. The conjugation of (DTPA)_n_-trastuzumab with IRDye 800CW was performed with a commercially available kit as described by Sampath et al. (12). This reaction had a typical yield of 90%, and a spectrophotometric analysis of the final product from this reaction revealed that 7–10 molecules (m) of IRDye800CW were conjugated to (DTPA)_n_-trastuzumab to yield (DTPA)_n_-trastuzumab-(IRDye 800CW)_m_.

To label (DTPA)_n_-trastuzumab-(IRDye 800CW)_m_ with ^111^In, indium chloride in sodium acetate buffer was mixed with (DTPA)_n_-trastuzumab-(IRDye 800CW)_m_ in phosphate-buffered saline (PBS) for 30 min to yield ^111^In-trastuzumab-IRDye 800CW (12). The procedure used for purification of the radiopharmaceutical and the radiochemical purity were not reported. Specific activity of the dual-labeled MAb was reported to be 7.4 MBq/nmol (0.2 mCi/nmol).

Stability of the dual-labeled MAb was determined in cell culture medium containing 10% fetal bovine serum for 24 h at 37°C (12). High-performance liquid chromatography (HPLC) was used to detect any degradation products produced from the dual-labeled MAb during the stability study. The column used for the HPLC analysis of the degradation products was not reported. ^111^In-Trastuzumab-IRDye 800CW was reported to be stable for 14 d at 4°C, but exposure to serum at 37°C resulted in ~6%/d degradation of the radiopharmaceutical as determined with HPLC.

For use as a control, human IgG was dual-labeled to yield ^111^In-(DTPA)_p_-IgG-(IRDye 800CW)_q_ as described above (12). The number of DTPA molecules (p) conjugated to the IgG was determined with mass spectroscopy; however, the number of DTPA residues conjugated to each IgG molecule was not reported. The ratio of IRDye 800CW to MAb (q) was calculated with spectrophotometric analysis, and for a single batch of ^111^In-(DTPA)_p_-IgG-(IRDye 800CW)_q_ the dye/MAb ratio was reported to be ~3. The yield of this reaction was reported to be 90%. Specific activity and stability of the dual-labeled human IgG was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

Human breast cancer cell lines SKBr3 (overexpress HER2) and MDA-MB-231 (have negligible expression of HER2) were used to study the in vitro binding characteristics of (DTPA)_n_-trastuzumab-(IRDye 800CW)_m_ and IRDye 800CW (12). For competitive binding studies the SKBr3 cells were treated with trastuzumab or human IgG for 30 min at 37°C before exposure to (DTPA)_n_-trastuzumab-(IRDye 800CW)_m_ for 1 h at the same temperature. The cells were then washed twice with PBS and stained with Sytol Green (in ethanol) for 15 min to fix the cells and stain the nuclei. Only the SKBr3 cells were reported to bind (DTPA)_n_-trastuzumab-(IRDye 800CW)_m_ as confirmed with confocal microscopy. SKBr3 cells pretreated with unlabeled trastuzumab, but not with human IgG, showed no binding of (DTPA)_n_-trastuzumab-(IRDye 800CW)_m_. Only a negligible amount of the free IRDye 800CW was reported to bind to the SKBr3 cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+trastuzumab+IRDye800+rodentia)]

For the in vivo imaging studies in nude mice, a derivative of the SKBr3 cells designated SKBr3-luc, which expresses the firefly luciferase (luc) gene, was used to develop xenograft tumors in nude mice (12). The SKBr3-luc cells were used to monitor the growth of xenograft tumors with bioluminescence imaging in the animals. Whole-body fluorescence imaging was performed 24 and 48 h after the respective administration of ^111^In-trastuzumab-IRDye 800CW (n = 3 animals), ^111^In-IgG-IRDye 800CW (n = 5 animals), and free IRDye 800CW (n = 5 animals) to the different groups of mice. For the competition studies, five mice were pretreated with 200-fold molar excess of unlabeled trastuzumab for 24 h before administration of ^111^In-trastuzumab-IRDye 800CW. At 48 h, whole-body fluorescence imaging data produced a tumor/muscle ratio (TMR) for mice injected with ^111^In-trastuzumab-IRDye 800CW of 2.25 ± 0.2 compared with TMR of 1.35 ± 0.1 for animals administered ^111^In-IgG-IRDye 800CW. Animals treated with the free IRDye 800CW had a TMR of 1.44 ± 0.18. The TMR of animals pretreated with trastuzumab was significantly lower (P = 0.0048) compared with animals treated with ^111^In-trastuzumab-IRDye 800CW. Single-photon emission computed tomography (SPECT) was performed on animals 48 h after the treatment with ^111^In-trastuzumab-IRDye 800CW. The TMR of the tumor region was reported to be 2.66, and whole-body scintigraphy images of the animals also showed a similar trend with a TMR of 2.17.

Dissection of the major organs 48 h after treatment of the animals with the respective imaging agents, except IRDye 800CW, for ex vivo imaging revealed that fluorescence was found primarily in the liver and kidneys of the animals (12). Fluorescence with IRDye 800CW was mainly in the kidneys, and no accumulation of the fluorescent dye was observed in the liver. A comparison of the TMRs between the nuclear and optical modalities showed that the TMRs observed with optical imaging were significantly (P = 0.001) higher than those observed with SPECT. However, a statiscally high (P = 0.0001) correlation, with an R value of 0.9476, was reported between the TMRs determined with the optical and SPECT modalities for the dual-labeled trastuzumab (^111^In-trastuzumab-IRDye 800CW).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+trastuzumab+IRDye800+Non+Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+trastuzumab+IRDye800+Non+Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+trastuzumab+IRDye800+human+studies)]

No references are currently available.

## Supplemental Information

### NIH Support

Work presented in this chapter was supported by National Institutes of Health Grants P50 CA58183, R01 EB003132, and R01 CA112679.

### References

1 Milanezi F., Carvalho S., Schmitt F.C. (2008). EGFR/HER2 in breast cancer: a biological approach for molecular diagnosis and therapy. Expert Rev Mol Diagn.
2 Park J.W., Neve R.M., Szollosi J., Benz C.C. (2008). Unraveling the biologic and clinical complexities of HER2. Clin Breast Cancer.
3 Azim H., Azim H.A. (2008). Targeting Her-2/neu in breast cancer: as easy as this!. Oncology.
4 Medina P.J., Goodin S. (2008). Lapatinib: a dual inhibitor of human epidermal growth factor receptor tyrosine kinases. Clin Ther.
5 Stipsanelli E., Valsamaki P. (2005). Monoclonal antibodies: old and new trends in breast cancer imaging and therapeutic approach. Hell J Nucl Med.
6 Barrett T., Koyama Y., Hama Y., Ravizzini G., Shin I.S., Jang B.S., Paik C.H., Urano Y., Choyke P.L., Kobayashi H. (2007). In vivo diagnosis of epidermal growth factor receptor expression using molecular imaging with a cocktail of optically labeled monoclonal antibodies. Clin Cancer Res.
7 Koyama Y., Hama Y., Urano Y., Nguyen D.M., Choyke P.L., Kobayashi H. (2007). Spectral fluorescence molecular imaging of lung metastases targeting HER2/neu. Clin Cancer Res.
8 Copland J.A., Eghtedari M., Popov V.L., Kotov N., Mamedova N., Motamedi M., Oraevsky A.A. (2004). Bioconjugated gold nanoparticles as a molecular based contrast agent: implications for imaging of deep tumors using optoacoustic tomography. Mol Imaging Biol.
9 Tada H., Higuchi H., Wanatabe T.M., Ohuchi N. (2007). In vivo real-time tracking of single quantum dots conjugated with monoclonal anti-HER2 antibody in tumors of mice. Cancer Res.
10 Artemov D., Mori N., Okollie B., Bhujwalla Z.M. (2003). MR molecular imaging of the Her-2/neu receptor in breast cancer cells using targeted iron oxide nanoparticles. Magn Reson Med.
11 Huh Y.M., Jun Y.W., Song H.T., Kim S., Choi J.S., Lee J.H., Yoon S., Kim K.S., Shin J.S., Suh J.S., Cheon J. (2005). In vivo magnetic resonance detection of cancer by using multifunctional magnetic nanocrystals. J Am Chem Soc.
12 Sampath L., Kwon S., Ke S., Wang W., Schiff R., Mawad M.E., Sevick-Muraca E.M. (2007). Dual-labeled trastuzumab-based imaging agent for the detection of human epidermal growth factor receptor 2 overexpression in breast cancer. J Nucl Med.
13 Tang Y., Wang J., Scollard D.A., Mondal H., Holloway C., Kahn H.J., Reilly R.M. (2005). Imaging of HER2/neu-positive BT-474 human breast cancer xenografts in athymic mice using (111)In-trastuzumab (Herceptin) Fab fragments. Nucl Med Biol.